# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene glycol 12 anti–tumor-associated glycoprotein 72 diabody

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-polyethylene glycol 12 anti–tumor-associated glycoprotein 72 diabody
Abbreviated name: | ^64^Cu-PEG12 AVP04-07
Synonym: | ^64^Cu-DOTA-PEG12-Cys-VS-AVP04-07
Agent Category: | Antibodies (diabodies)
Target: | Tumor-associated glycoprotein 72 (TAG-72)
Target Category: | Antigens
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=antibody+fragments+and+molecular+imaging)]

The ^64^Cu-labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA)-polyethylene glycol 12 (PEG12) anti–tumor-associated glycoprotein 72 (TAG-72) diabody conjugate, abbreviated as ^64^Cu-PEG12 AVP04-07, is a positron emission tomography (PET) tracer that has been developed by Li et al. for imaging tumors by targeting overexpressed TAG-72 antigen (1). Conjugation of monodispersed PEG to antibody fragments has been shown to be an effective approach to reduce kidney retention and increase the tumor uptake of antibody fragments (1). The half-life (t_1/2_) of ^64^Cu is 12.7 h.

Antibody fragments such as diabodies and minibodies are ideal for molecular imaging because of their compact size and efficient antigen binding (1-4). However, most radiometal-labeled antibody fragments exhibit high kidney retention, which leads to decreased absolute tumor uptake (5-7). In the case of ^64^Cu, which has greater tumor retention than radioiodine labels, the advantage is offset by prolonged kidney retention. Use of radioiodine labels results in decreased kidney uptake, but at the expense of lower tumor uptake (1, 8, 9). An approach to avoid the kidney retention issue is to increase the apparent molecular weight of antibody fragments through attachment of PEG (5). This approach has been successfully applied to the engineered antibody fragments against carcinoembryonic antigen (CEA), CD3, and others (5, 10). Increased tumor retention, longer serum t_1/2_, and decreased kidney uptake have been observed for PEGylated fragments compared with non-PEGylated forms (5, 11). Li et al. reported that attachment of DOTA and PEG3400 to anti-CEA diabody can significantly reduce kidney uptake of the diabody compared with kidney uptake of the parental diabody while preserving high tumor uptake (5, 12). They further generated a PEGylated (PEG3400) anti-TAG-72 diabody (AVP04-07-PEG3400), which reduced kidney retention to levels usually seen with intact immunoglobulin G. Kidney uptake appears to be a function of apparent molecular size (as modified by PEG) and other less defined factors intrinsic to a diabody (1). However, PEG3400 is less than ideal for clinical use because of its inherent polydispersity. Oversubstitution may also inhibit the immunoreactivity of the antibody fragments. In the case of anti-CEA diabody, Li et al. showed that it is necessary to limit the number of PEG3400 particles to approximately one per monomer (5). Li et al. therefore evaluated the effect of monodispersed PEG on the kidney retention and tumor uptake of anti-TAG-72 diabody (1). The investigators synthesized monodispersed PEG (DOTA-PEG12-Cys-VS, where Cys-VS is vinyl sulfone conjugated to the thiol of cysteine) and conjugated this to the amino groups on the anti-TAG-72 diabody (named as PEG12 AVP04-07). Biodistribution studies with ^111^In-labeled PEG12 AVP04-07 demonstrated low kidney uptake without reduction of the tumor uptake and tumor/blood ratio. Positron emission tomography (PET) imaging with ^64^Cu-PEG12 AVP04-07 showed high-contrast tumor images in animal models within 24 h after injection (1).

### Related Resource Links:

- MICAD chapters on TAG-72 antigen (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=anti-TAG-72+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- MICAD chapters on antibody fragments (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=antibody+fragments+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Nucleotide sequences of TAG-72 (http://www.ncbi.nlm.nih.gov/nucleotide/?term=TAG-72)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Li+and+TAG-72+diabody)]

The parental AVP04-07 diabody was generated on the basis of the V-domains from the parent CC49 antibody and the derivative single-chain Fv (scFv) fragments (1, 13). The scFv fragments are orientated as V_H_–V_L_ (where V_H_ and V_L_ are the variable domains of heavy and light chains, respectively) joined by a G_4_S linker and have a C-terminal His_6_ tail. The apparent molecular weight was 52.5 kDa for the AVP04-07 diabody. To construct PEG12 AVP04-07, monodispersed DOTA-PEG12-Cys-VS was first synthesized by coupling N-FMOC-amido-PEG12 acid to Cys-polystyrene Wang resin, followed by reaction with a 10-molar excess of VS. Conjugation of the DOTA-PEG12-Cys-VS to the surface lysines of the diabody was carried out at pH 9.0 at a molar ratio of 50:1 and 20:1, respectively.

Radiometal labeling was performed with ^111^InCl_3_ or ^64^CuCl_2_ as described in previous reports (1, 12). The radiolabeled materials were purified on Superdex-75 columns. The degree of substitution was estimated to be 1.7 PEGs per monomer for the 20:1 conjugate and 3.0 PEGs per monomer for the 50:1 conjugate. When the conjugates were labeled with ^111^In, the 20:1 conjugate gave 8.3% incorporation and the 50:1 conjugate gave 92% incorporation. The radiolabeled 50:1 conjugate was used for in vivo studies.

The ^111^In- and ^64^Cu-labeled DOTA-Cys-VS-PEG3400-AVP04-07 conjugates (referred to as ^111^In- and ^64^Cu-AVP04-07-PEG3400) and DOTA-Cys-VS-PEG27-AVP04-07 conjugates (referred to as ^111^In-PEG27 AVP04-07 and ^64^Cu-PEG27 AVP04-07; MICAD chapter on ^64^Cu-PEG27 AVP04-07 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) were synthesized similarly. The apparent molecular weight was 105 kDa for the PEG3400 derivatives, but the apparent molecular weight was not described in detail for the PEG12 and PEG27 conjugates. The radiolabeling yields were typically 70%–90% for the PEG conjugates.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Li+and+TAG-72+diabody)]

Binding of AVP04-07 diabody to the TAG-72 antigen was determined with bovine submaxillary mucin in a column shift assay (Superdex 200) (1). The AVP04-07 diabody showed >99% immunoreactivity. No data were described for the immunoreactivity of ^111^In- and ^64^Cu-labeled conjugates.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Li+and+TAG-72+diabody)]

A biodistribution study was performed in athymic nude mice bearing LS-174T xenografts (1). In the case of ^111^In-AVP04-07-PEG3400, kidney uptake was 8.4% injected dose per gram tissue (ID/g) at 24 h after injection; uptake was 98% ID/g for the non-PEGylated form. The large reduction of kidney uptake with PEGylation was accompanied by an increase in tumor uptake from 22% ID/g (non-PEGylated) to 46% ID/g (PEGylated) at 24 h. The increased tumor retention is evidently due to the prolonged blood clearance of the PEGylated diabody (t_1/2β_ = 36 h) versus the non-PEGylated diabody (t_1/2β_ = 18 h). Biodistribution results for ^111^In-PEG12 AVP04-07 were nearly equivalent to those for the PEG3400 and PEG27 derivatives. Notably, kidney uptake was initially higher for the PEG12 conjugate (13.4% ID/g) than for the PEG27 conjugate, but fell to lower levels (6.1% ID/g) by 96 h, whereas tumor uptake and blood clearance were nearly identical for the PEG12 and the PEG27 conjugates.

PET imaging demonstrated modest tumor uptake (19.6% ID/g at 46 h) and high kidney uptake (37.4% ID/g at 46 h) for the ^64^Cu-labeled non-PEGylated AVP04-07 within 2 days after injection. In contrast, ^64^Cu-PEG12 AVP04-07 showed relatively little kidney uptake (6.7% ID/g at 46 h) over the same period and high tumor uptake (49.3% ID/g at 46 h) as early as 21–22 h after injection. The tumor/blood ratio reached 9:1 at 46 h after injection. The results with the ^64^Cu-labeled conjugate were similar to those obtained with the ^111^In-labeled conjugate. The best imaging predicted with imaging figure of merit was at 10 h for the ^64^Cu-labeled non-PEGylated diabody and at 20 h for the ^64^Cu-labeled PEG12 version. For the ^111^In-labeled PEG12 conjugate, imaging was optimal at 30–40 h.

In summary, the PEGylated diabody outperformed the non-PEGylated form in terms of both absolute tumor uptake and tumor/blood ratio for both ^111^In and ^64^Cu labels. The results obtained by Li et al. suggested that even PEGs of modest molecular size are efficient in reducing kidney uptake and that the choice of radiometal labels has little effect on the biodistribution. Monodispersed DOTA-PEGylated diabody conjugates are more suitable for imaging of human TAG-72–positive tumors (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Li L., Turatti F., Crow D., Bading J.R., Anderson A.L., Poku E., Yazaki P.J., Williams L.E., Tamvakis D., Sanders P., Leong D., Raubitschek A., Hudson P.J., Colcher D., Shively J.E. (2010). Monodispersed DOTA-PEG-Conjugated Anti-TAG-72 Diabody Has Low Kidney Uptake and High Tumor-to-Blood Ratios Resulting in Improved 64Cu PET. J Nucl Med.
2 Kortt A.A., Dolezal O., Power B.E., Hudson P.J. (2001). Dimeric and trimeric antibodies: high avidity scFvs for cancer targeting. Biomol Eng.
3 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
4 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
5 Li L., Yazaki P.J., Anderson A.L., Crow D., Colcher D., Wu A.M., Williams L.E., Wong J.Y., Raubitschek A., Shively J.E. (2006). Improved biodistribution and radioimmunoimaging with poly(ethylene glycol)-DOTA-conjugated anti-CEA diabody. Bioconjug Chem.
6 Li L., Olafsen T., Anderson A.L., Wu A., Raubitschek A.A., Shively J.E. (2002). Reduction of kidney uptake in radiometal labeled peptide linkers conjugated to recombinant antibody fragments. Site-specific conjugation of DOTA-peptides to a Cys-diabody. Bioconjug Chem.
7 Trejtnar F., Laznicek M. (2002). Analysis of renal handling of radiopharmaceuticals. Q J Nucl Med.
8 Schibli R., Schubiger P.A. (2002). Current use and future potential of organometallic radiopharmaceuticals. Eur J Nucl Med Mol Imaging.
9 Lin, X., J. Xie, and X. Chen, Protein-based tumor molecular imaging probes. Amino Acids, 2010
10 Olafsen T., Cheung C.W., Yazaki P.J., Li L., Sundaresan G., Gambhir S.S., Sherman M.A., Williams L.E., Shively J.E., Raubitschek A.A., Wu A.M. (2004). Covalent disulfide-linked anti-CEA diabody allows site-specific conjugation and radiolabeling for tumor targeting applications. Protein Eng Des Sel.
11 Delgado C., Pedley R.B., Herraez A., Boden R., Boden J.A., Keep P.A., Chester K.A., Fisher D., Begent R.H., Francis G.E. (1996). Enhanced tumour specificity of an anti-carcinoembrionic antigen Fab' fragment by poly(ethylene glycol) (PEG) modification. Br J Cancer.
12 Li L., Bading J., Yazaki P.J., Ahuja A.H., Crow D., Colcher D., Williams L.E., Wong J.Y., Raubitschek A., Shively J.E. (2008). A versatile bifunctional chelate for radiolabeling humanized anti-CEA antibody with In-111 and Cu-64 at either thiol or amino groups: PET imaging of CEA-positive tumors with whole antibodies. Bioconjug Chem.
13 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.